# 2-(2-(3-[^11^C]Methoxyphenyl)ethynyl)pyridine

Chemical name: | 2-(2-(3-[^11^C]Methoxyphenyl)ethynyl)pyridine
Abbreviated name: | [^11^C]M-MPEP
Synonym:
Agent Category: | Compound
Target: | Metabotropic glutamate subtype 5 (mGlu5) receptor (mGluR5 or mGluR_5_)
Target Category: | Receptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal /contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=metabotropic+glutamate+receptor+subtype+5+PET+ligand)]

2-(2-(3-[^11^C]Methoxyphenyl)ethynyl)pyridine ([^11^C]M-MPEP) is a radioligand developed for positron emission tomography (PET) imaging of metabotropic glutamate (mGlu) receptor subtype 5 (mGluR5 or mGluR_5_) in the central nervous system (CNS) (1). ^11^C is a positron emitter with a physical half-life (t_½_) of 20.3 min.

Glutamate is a major excitatory neurotransmitter at CNS synapses. Many neuroanatomical CNS projection pathways contain glutamatergic neurons (2). Glutamate produces its excitatory effects by acting on cell-surface ionotropic glutamate or mGluRs (3). The mGluRs are G-protein–coupled receptors, and the eight mGluR subtypes are further subdivided into three groups. The group I receptors include mGluR1 and mGluR5, and they are found predominantly in postsynaptic locations. The mGluR5s are found with high to moderate density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, hippocampus, and dorsal horn of the spinal cord, whereas the density in the cerebellum is low. These receptors are coupled to phospholipase C, and they up- or downregulate neuronal excitability. They have been implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal. These receptors are also involved in the modulation of various pain states, which makes them attractive targets for therapeutic drug development.

PET and single-photon emission computed tomography imaging of radioligands that target mGluR5s are used to visualize and study the CNS mGluR5s in normal and pathological states. Some mGluR5 antagonists have been successfully labeled, but their in vivo visualization has been hampered by high lipophilicity, unfavorable brain uptake kinetics, or high metabolism (4, 5). MPEP and its methyl analog M-MPEP have been identified as potent and highly selective noncompetitive antagonists for mGlu5 (1, 6). Yu et al. (1) synthesized [^11^C]M-MPEP and demonstrated the feasibility of using it as an imaging ligand for in vivo PET imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+synthesis)]

Gasparini et al. (6) reported the synthesis of the phenolic precursor 3-(2-(6-methylpyridin-2-yl)ethynyl)-phenol of M-MPEP. Briefly, 2,6-dimethyl-pyridine and 3-hydroxy-benzaldehyde were used as starting materials. They were condensed in acetic anhydride at 165ºC for 3.5 h to form a styrene derivative. This intermediate compound was dibrominated in the dark at room temperature. This dibrominated intermediate was then converted to 3-(2-(6-methylpyridin-2-yl)ethynyl)-phenol using potassium tert-butylate in potassium hydroxide (KOH), crown ether 18C6, and tetrahydrofuran at 50ºC for 1.5 h.

Yu et al. (1) reported the radiosynthesis of [^11^C]M-MPEP by radiolabeling this phenolic precursor with ^11^C methyl iodide ([^11^C]CH_3_I) under basic conditions. [^11^C]CH_3_I was prepared from ^11^CO_2_ with the use of the ^14^N(p,α)^11^C reaction. The best yield conditions were obtained with KOH as the base. In this radiolabeling reaction, 4–10 mg of solid KOH powder was added to 0.5–1.0 mg of the precursor dissolved in dimethyl sulfoxide before [^11^C]CH_3_I was added to the reaction mixture. The mixture was heated at 90ºC for 6 min. The radioligand was purified by high-performance liquid chromatography (HPLC). The radiochemical purity was >98.4 ± 1.3% (n = 7), and the specific activity was 23.2 ± 4.7 GBq/μmol (857 ± 173 mCi/μmol). The radiochemical yield was 3.1 ± 1.5 GBq (84.7 ± 39.6 mCi) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+rodentia)]

Yu et al. (1) performed dynamic PET imaging of [^11^C]M-MPEP in male rats (n = 13). Each anesthetized rat received 108.52 ± 73.70 MBq (2.93 ± 2.00 mCi) in 0.72 ± 0.49 μg [^11^C]M-MPEP (2–3 nM in 0.1 ml or ~3.4 nmol calculated from the mean specific activity of 0.86 mCi/nmol) by intravenous administration. Imaging for 1 h showed that the radioligand was eliminated from the body through gastrointestinal pathways; no radioactivity was observed in the bladder. Maximum radioactivity accumulation occurred within 1–2 min except in the pancreas and ductus choreolus, where the radioactivity accumulated for up to 50 min. In the brain, the highest radioactivity level was in the olfactory area, followed by the hippocampus, cortex, and striatum. The authors suggested that this distribution pattern appeared to match the brain mGluR5 densities in rats (7). The olfactory bulb/cerebellum ratio of radioactivity reached a maximum of 4.2 at 40 min. The radioactivity levels (n = 13) of the whole brain in percentage of injected dose per cubic centimeter (% ID/cc) obtained from volumetric region-of-interest image analysis were 0.187 ± 0.130 (5 min), 0.106 ± 0.070 (10 min), 0.072 ± 0.046 (20 min), 0.057 ± 0.034 (30 min), 0.049 ± 0.029 (40 min), 0.044 ± 0.025 (50 min), and 0.045 ± 0.029 (60 min). The radioactivity levels (% ID/cc) of the olfactory bulb were 0.390 ± 0.316 (5 min), 0.302 ± 0.246 (10 min), 0.244 ± 0.194 (20 min), 0.192 ± 0.145 (30 min), 0.163 ± 0.120 (40 min), 0.148 ± 0.109 (50 min), and 0.122 ± 0.103 (60 min). The [^11^C]M-MPEP radioactivity level was reversible in all areas of the body. When a blocking dose of 10 mg/kg unlabeled MPEP was administered 5 min before the radioligand injection (79.18 ± 56.98 MBq (2.14 ± 1.54 mCi) in 0.52 ± 0.38 μg (~2.49 nmol calculated from the mean specific activity of 0.86 mCi/nmol)), the radioactivity levels (n = 8) of the olfactory lobe were decreased by 59.7% at 5 min and 29.4% at 40 min. In the other parts of the brain, MPEP decreased radioactivity levels of [^11^C]M-MPEP in the early time points. The decrease was 28.9% in the whole brain, 44.8% in the cortex, 14.0% in the hippocampus, and 28.7% in the striatum at 5 min. At the later time points, the radioactivity levels of [^11^C]M-MPEP increased moderately. Outside the brain, MPEP decreased the [^11^C]M-MPEP radioactivity level in the intestine at 10 min. The authors suggested that the effect of unlabeled MPEP administration was time- and dose-dependent.

In the in vivo metabolism study, [^11^C]M-MPEP was shown by HPLC analysis to be rapidly metabolized after administration (1). The percentage of the radioligand remaining intact in the plasma after administration (n = 2) was 44.5 ± 0.8% at 5 min, 32.7 ± 5.9% at 10 min, and 21.4 ± 0.5% at 20 min. No lipophilic metabolite from [^11^C]M-MPEP was found.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(metabotropic+glutamate+receptor+subtype+5+PET+ligand)+AND+human)]

No publication is currently available.

## NIH Support

NIH/NIBIB grant EB01850.

## References

1 Yu M., Tueckmantel W., Wang X., Zhu A., Kozikowski A.P., Brownell A.L. (2005). Methoxyphenylethynyl, methoxypyridylethynyl and phenylethynyl derivatives of pyridine: synthesis, radiolabeling and evaluation of new PET ligands for metabotropic glutamate subtype 5 receptors. Nucl Med Biol.
2 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
3 Slassi A., Isaac M., Edwards L., Minidis A., Wensbo D., Mattsson J., Nilsson K., Raboisson P., McLeod D., Stormann T.M., Hammerland L.G., Johnson E. (2005). Recent advances in non-competitive mGlu5 receptor antagonists and their potential therapeutic applications. Curr Top Med Chem.
4 Ametamey S.M., Kessler L.J., Honer M., Wyss M.T., Buck A., Hintermann S., Auberson Y.P., Gasparini F., Schubiger P.A. (2006). Radiosynthesis and Preclinical Evaluation of 11C-ABP688 as a Probe for Imaging the Metabotropic Glutamate Receptor Subtype 5. J Nucl Med.
5 Patel S., Ndubizu O., Hamill T., Chaudhary A., Burns H.D., Hargreaves R., Gibson R.E. (2005). Screening cascade and development of potential Positron Emission Tomography radiotracers for mGluR5: in vitro and in vivo characterization. Mol Imaging Biol.
6 Gasparini F., Andres H., Flor P.J., Heinrich M., Inderbitzin W., Lingenhohl K., Muller H., Munk V.C., Omilusik K., Stierlin C., Stoehr N., Vranesic I., Kuhn R. (2002). [(3)H]-M-MPEP, a potent, subtype-selective radioligand for the metabotropic glutamate receptor subtype 5. Bioorg Med Chem Lett.
7 Shigemoto R., Nomura S., Ohishi H., Sugihara H., Nakanishi S., Mizuno N. (1993). Immunohistochemical localization of a metabotropic glutamate receptor, mGluR5, in the rat brain. Neurosci Lett.